# [^99m^Tc]Cyclo(L-homocysteinyl-N-methyl-L-phenylalanyl-L-tyrosyl-D-tryptophyl-L-lysyl-L-valyl), (1‡1´)-sulfide with 3-[(mercaptoacetyl)amino]-L-alanyl-L-lysyl-L-cysteinyl-L-lysinamide

Chemical name: | [^99m^Tc]Cyclo(L-homocysteinyl-N-methyl-L-phenylalanyl-L-tyrosyl-D-tryptophyl-L-lysyl-L-valyl), (1‡1´)-sulfide with 3-[(mercaptoacetyl)amino]-L-alanyl-L-lysyl-L-cysteinyl-L-lysinamide
Abbreviated name: | [^99m^Tc]Depreotide
Synonym: | P829; Neospect; Neotect; Neo Tect
Agent Category: | Peptide
Target: | Somatostatin receptors
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Structure of Depreotide

## Background

[PubMed]

Somatostatin receptors (SSTRs) are implicated in the development of various cancerous tumors of endocrine origin, including those found in the lungs (1, 2). Five types of SSTRs, designated as SSTR1 to SSTR5, have been identified, and the frequency and expression pattern of each receptor type were reported to change with the tumor type (3, 4). On the basis of histological criteria, endocrine carcinomas may show low or intermediate differentiation or could be of the nondifferentiated type; individuals with the latter type of tumor usually have a poor prognosis (1, 5). Activation of the SSTR by the binding of somatostatin (SS) usually inhibits the production of hormones from various glands, and investigators have attempted to use SS for the treatment of various diseases, including endocrine cancers. However, SS has a short plasma half-life because of rapid enzymatic degradation, which makes SS ineffective for such therapy (6). Therefore, the development of SS analogs that are resistant to enzymatic degradation but have a biological activity similar to SS has led to the evaluation of such analogs for the diagnosis and treatment of cancerous tumors of endocrine origin (7-9).

Octreotide, a synthetic analog of SS, was approved by the United States Food and Drug Administration (FDA) for the treatment of hormone hypersecretion in individuals suffering from acromegaly and gastropancreatic and carcinoid tumors (10). This molecule was subsequently radiolabeled with isotopes of indium (^111^In) and iodine (^123^I) and has been shown to be a useful agent for the detection of small primary neuroendocrine tumors or their metastasized forms, which are visualized by conventional means (11, 12). However, although these radionuclides are available yet they are expensive to produce. Because radioactive technetium (^99m^Tc) is cheaper to produce and yields better images compared with ^111^In- or ^123^I-labeled compounds, Vallabhajosula et al. decided to use ^99m^Tc to label SS analogs for preclinical evaluation in rats bearing SS-positive tumors (13). One such SS analog, depreotide, also known as peptide P829, is a tetrapeptide attached to a cyclic hexapeptide that was labeled with ^99m^Tc to produce [^99m^Tc]Depreotide. [^99m^Tc]Depreotide has been shown to have a high affinity for SSTR2, SSTR3, and SSTR5 (14). The peptide is commercially available as a kit in Europe and is approved for scintigraphic imaging of malignant lung tumors in conjunction with computed tomography (CT) (9). In the United States this radiochemical is approved by the FDA for the evaluation of indeterminate nodules in the lungs (15).

## Synthesis

[PubMed]

The synthesis of depreotide was described by Vallabhajosula et al. (13). Briefly, the peptide was synthesized using solution and solid-phase peptide synthesis techniques with F-α-Fmoc chemistry. A Delta-pak C_18_ column was used for preparative purification of the peptide with reverse-phase high-performance liquid chromatography (RP-HPLC). The purified peptide was lyophilized, and its identity was confirmed with RP-HPLC on a C_18_ column and with fast-atom bombardment mass spectrometry.

After dissolving the peptide in normal saline the ligand exchange method with ^99m^Tc-glucoheptonate (in 50% ethanol) was used to label depreotide with ^99m^Tc (13). The reaction mixture was incubated at room temperature for 20 min, and the radiochemical purity (RCP) of [^99m^Tc]depreotide was determined with instant thin-layer chromatography (ITLC). The Rf values of the labeled product and the various components used to produce the radiochemical were not reported by the investigators, but [^99m^Tc]depreotide was reported to remain immobile while [^99m^Tc]glucoheptonate was mobile with the developing solvent under the conditions used to perform ITLC (13). The RCP of [^99m^Tc]depreotide was also determined with RP-HPLC. The radiochemical yield and RCP of the labeled peptide were each reported to be >90%, and no further purification was performed before use (13). The specific activity of [^99m^Tc]depreotide was reported to be routinely 2.2 TBq/mmol (60 Ci/mmol).

Depreotide is commercially available as a lyophilized product in the United States for use as an injectable after labeling with ^99m^Tc (as sodium pertechnetate). The lyophilized vial preparation (contains no antimicrobial preservative) contains depreotide, stannous chloride, edentate disodium dehydrate, sodium iodide, and sodium hydroxide or hydrochloric acid to adjust the pH to 7.4 prior to lyophilization. After freeze-drying, the contents are sealed under nitrogen with a rubber closure (16). The kit may be stored at 2–8°C, and the reconstituted injection solution may be stored at 20–25°C for use within 6 h after reconstitution.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

The in vitro binding characteristics of [^99m^Tc]P829 were studied in several primary human tumors, including those originating from small cell and non-small cell lung cancer cells, melanomas, breast cancer, intestinal adenocarcinomas, pheochromocytomas, carcinoids, different tumor cell lines, and COS7 cells respectively transfected with human SSTR (hSSTR) subtypes 1 to 5 (14). The radiolabeled peptide bound with high affinity to the various tumor cells and had dissociation constant values of 2.5, 1.5, and 2.0 nM for hSSTR2, -3, and -5, respectively.

## Animal Studies

### Rodents

[PubMed]

Vallabhajosula et al. investigated the biodistribution of [^99m^Tc]P829 and [^111^In]DTPA-octreotide after a dual injection of the radiochemicals in Lewis rats bearing CA20948 tumors (n = 3 animals for each group) (13). The animals were killed 90 min after the injection and the percent injected dose per gram tissue (% ID/g) was determined for the tumors and several other tissues. In this model, a higher uptake of [^99m^Tc]P829 by the tumors was reported compared with [^111^In]DTPA-octreotide, but the tumor/muscle ratios were comparable for both tracers. The investigators reported a reduced uptake of [^99m^Tc]P829 by the tumors when the tracer was co-injected into the animals with increasing concentrations of the non-radioactive peptide (13).

The biodistribution of [^99m^Tc]depreotide, [^111^In]DTPA-octreotide, and [^177^Lu]DOTA-Tyr3-octreotate was compared in a small cell lung cancer xenografted nude mouse model (17). Mice were injected simultaneously with [^99m^Tc]depreotide and [^111^In]DTPA-octreotide, and the activity concentration per gram tissue (% IA/g) was determined in the tumors and normal tissue between 2 and 24 h after administration (n = 3–5 animals per time point). Results obtained from this study were compared with those obtained with [^177^Lu]DOTA-Tyr3-octreotate from an earlier study that used the same animal model (18). In this earlier study, [^111^In]DTPA-octreotide was reported to show a higher % IA/g compared with [^99m^Tc]depreotide (P < 0.05), but at 24 h after injection [^177^Lu]DOTA-Tyr3-octreotate had the highest tumor uptake. A significantly higher uptake of [^99m^Tc]depreotide was observed in the heart, lungs, liver, salivary glands, spleen, and bone marrow compared with [^111^In]DTPA-octreotide at all time points. The lower tumor/lung and tumor/liver ratios observed with [^99m^Tc]depreotide compared with [^111^In]DTPA-octreotide suggested that [^99m^Tc]depreotide may yield a lower detection rate of small cell lung cancer compared with [^111^In]DTPA-octreotide. The investigators reported no blocking studies for [^99m^Tc]depreotide with this animal model (17).

### Other Non-Primate Mammals

[PubMed]

Vallabhajosula et al. studied the biodistribution of [^99m^Tc]P829 normal rabbits (the number of animals used for this study was not provided by the investigators) (13). The animals were injected with the radiochemical, and serial static images were obtained every hour for up to 4 h. The investigators reported that 30% of [^99m^Tc]P829 activity was observed in the kidney, 20% in the urinary bladder, and <5% in the gastrointestinal tract of the animals.

### Non-Human Primates

[PubMed]

No references are currently available.

## Human Studies

[PubMed]

The use of [^99m^Tc]depreotide for the detection of various cancers in humans, including bone metastasis observed in individuals with lung cancer, was evaluated by Mena et al. (19). All 20 patients enrolled in the study were diagnosed with lung cancer with bone metastasis as detected by conventional methods. The patients underwent scintigraphy with [^99m^Tc]hydroxyethylene diphosphonate ([^99m^Tc]HEDP) and [^99m^Tc]depreotide within 2 weeks. The bone lesions (n = 55) were classified as benign or malignant on the basis of clinical, imaging, and histological criteria. The investigators reported that 19 of the 20 patients showed an uptake of [^99m^Tc]depreotide in the primary tumors, and 90% of the 31 bone lesions (n = 28) that were classified as malignant with [^99m^Tc]HEDP were also detected with [^99m^Tc]depreotide. Of the 55 bone lesions, 24 lesions were classified as benign with [^99m^Tc]HEDP, and none of these lesions showed any [^99m^Tc]depreotide uptake. The investigators concluded that [^99m^Tc]depreotide could be used for the detection of malignant bone lesions if the primary lung tumors were positive for SSTRs (19).

Martins et al. used [^99m^Tc]depreotide scintigraphy for the evaluation of indeterminate pulmonary lesions detected with computed tomography (CT) in humans (n = 40 patients) (20). The 50 parenchymal lesions detected with CT were scored as positive or negative for the uptake of [^99m^Tc]depreotide; 97% of the malignant lesions were positive (i.e., sensitive) for [^99m^Tc]depreotide uptake, and 63% of the benign lesions were negative (i.e., specific) for the radiotracer. The benign lesions positive for [^99m^Tc]depreotide showed inflammation, infection, and bronchiectasis. The investigators noted a significant difference (P = 0.019) between malignant and benign lesions with semiquantitative analysis of the data. On the basis of the results obtained from this study, the investigators concluded that, because of its moderate specificity, it was best to use [^99m^Tc]depreotide in conjunction with clinical and radiological evaluation of patients to exclude malignancy with confidence.

In another study, the use of [^99m^Tc]depreotide and radioactive [^201^Tl]thallium chloride in single-photon emission computed tomography (SPECT) was compared in the characterization of pulmonary lesions (21). The investigators observed no difference in the diagnostic performance of the two radiochemicals and reported that the two tracers were equally effective in the determination of malignancies in the lung. However, the specificity of the two techniques was significantly improved by quantifying uptake of the two radiochemicals.

Cholewinski et al evaluated the use of [^99m^Tc]depreotide for the detection and staging of malignant lymphomas in 15 children (22). All patients were verified with other modalities (magnetic resonance imaging, ultrasound, or clinical examination) for staging before treatment with [^99m^Tc]depreotide. All children underwent whole-body scans and SPECT imaging of the chest and/or abdomen. In 11 patients, the number of lesions detected with [^99m^Tc]depreotide were higher than the number detected with CT. On the basis of [^99m^Tc]depreotide uptake. 3 patients were upstaged and none was downstaged.

In another study, [^99m^Tc]depreotide was evaluated for the detection of bone infection and inflammation in 23 patients with probable osteomyelitis who had already undergone a three-phase scintigraphic evaluation (23). Among these patients 12 of 12 individuals with osteomyelitis, 6 of 9 individuals with rheumatoid arthritis, and a single individual with femoral head osteonecrosis were positive for [^99m^Tc]depreotide uptake. Five individuals with no inflammation and 14 of 14 individuals with degenerative arthritis-osteoarthropathy were negative for [^99m^Tc]depreotide uptake. Individuals with bone infections (n = 5 patients) were positive for the radiotracer. It is pertinent to mention here that the use of [99mTc]depreotide for the detection of infection and inflammation is not an FDA approved indication for the radiochemical.

The use of [^99m^Tc]depreotide was also compared with the use of [^99m^Tc]methylenediphosphonate ([^99m^Tc]MDP) for the detection of bone metastasis in 12 breast cancer patients (24). The investigators concluded that although [^99m^Tc]depreotide was less sensitive than [^99m^Tc]MDP, it was more specific than [^99m^Tc]MDP in the measurement of the extent of bone metastasis in the breast cancer patients. In a study designed to compare the use of [^18^F]fluorodeoxyglucose ([^18^F]FDG) and [^99m^Tc]depreotide for the assessment of malignant lung lesions, the investigators concluded that [^18^F]FDG had a higher sensitivity and specificity compared with [^99m^Tc]depreotide (25).

## Supplemental Information

[Disclaimers]

## References

1 Pelosi G., Volante M., Papotti M., Sonzogni A., Masullo M., Viale G. (2006). Peptide receptors in neuroendocrine tumors of the lung as potential tools for radionuclide diagnosis and therapy. Q J Nucl Med Mol Imaging.
2 Asnacios A., Courbon F., Rochaix P., Bauvin E., Cances-Lauwers V., Susini C., Schulz S., Boneu A., Guimbaud R., Buscail L. (2008). Indium-111-pentetreotide scintigraphy and somatostatin receptor subtype 2 expression: new prognostic factors for malignant well-differentiated endocrine tumors. J Clin Oncol.
3 Mundschenk J., Unger N., Schulz S., Hollt V., Schulz S., Steinke R., Lehnert H. (2003). Somatostatin receptor subtypes in human pheochromocytoma: subcellular expression pattern and functional relevance for octreotide scintigraphy. J Clin Endocrinol Metab.
4 Fjallskog M.L., Ludvigsen E., Stridsberg M., Oberg K., Eriksson B., Janson E.T. (2003). Expression of somatostatin receptor subtypes 1 to 5 in tumor tissue and intratumoral vessels in malignant endocrine pancreatic tumors. Med Oncol.
5 Huang Q., Muzitansky A., Mark E.J. (2002). Pulmonary Neuroendocrine Carcinomas. A review of 234 cases and a statistical analysis of 50 cases treated at one institution using a simple clinicopathologic classification. Arch Pathol Lab Med.
6 Breeman W.A., Kwekkeboom D.J., de Blois E., de Jong M., Visser T.J., Krenning E.P. (2007). Radiolabelled regulatory peptides for imaging and therapy. Anticancer Agents Med Chem.
7 Forrer F., Waldherr C., Maecke H.R., Mueller-Brand J. (2006). Targeted radionuclide therapy with 90Y-DOTATOC in patients with neuroendocrine tumors. Anticancer Res.
8 Koukouraki S., Strauss L.G., Georgoulias V., Schuhmacher J., Haberkorn U., Karkavitsas N., Dimitrakopoulou-Strauss A. (2006). Evaluation of the pharmacokinetics of 68Ga-DOTATOC in patients with metastatic neuroendocrine tumours scheduled for 90Y-DOTATOC therapy. Eur J Nucl Med Mol Imaging.
9 Axelsson R., Herlin G., Baath M., Aspelin P., Kolbeck K.G. (2008). Role of scintigraphy with technetium-99m depreotide in the diagnosis and management of patients with suspected lung cancer. Acta Radiol.
10 Bauer W., Briner U., Doepfner W., Haller R., Huguenin R., Marbach P., Petcher T.J., Pless. (1982). SMS 201-995: a very potent and selective octapeptide analogue of somatostatin with prolonged action. Life Sci.
11 Bakker W.H., Krenning E.P., Breeman W.A., Kooij P.P., Reubi J.C., Koper J.W., de Jong M., Lameris J.S., Visser T.J., Lamberts S.W. (1991). In vivo use of a radioiodinated somatostatin analogue: dynamics, metabolism, and binding to somatostatin receptor-positive tumors in man. J Nucl Med.
12 Krenning E.P., Bakker W.H., Kooij P.P., Breeman W.A., Oei H.Y., de Jong M., Reubi J.C., Visser T.J., Bruns C., Kwekkeboom D.J., et al. (1992). Somatostatin receptor scintigraphy with indium-111-DTPA-D-Phe-1-octreotide in man: metabolism, dosimetry and comparison with iodine-123-Tyr-3-octreotide. J Nucl Med.
13 Vallabhajosula S., Moyer B.R., Lister-James J., McBride B.J., Lipszyc H., Lee H., Bastidas D., Dean R.T. (1996). Preclinical evaluation of technetium-99m-labeled somatostatin receptor-binding peptides. J Nucl Med.
14 Virgolini I., Leimer M., Handmaker H., Lastoria S., Bischof C., Muto P., Pangerl T., Gludovacz D., Peck-Radosavljevic M., Lister-James J., Hamilton G., Kaserer K., Valent P., Dean R. (1998). Somatostatin receptor subtype specificity and in vivo binding of a novel tumor tracer, 99mTc-P829. Cancer Res.
15 Menda Y., Kahn D. (2002). Somatostatin receptor imaging of non-small cell lung cancer with 99mTc depreotide. Semin Nucl Med.
16. Berlex, NeoTect kit for the preparationof technetium Tc99m depreotide injection. 2004.
17 Schmitt A., Bernhardt P., Nilsson O., Ahlman H., Kolby L., Forssell-Aronsson E. (2005). Differences in biodistribution between 99mTc-depreotide, 111In-DTPA-octreotide, and 177Lu-DOTA-Tyr3-octreotate in a small cell lung cancer animal model. Cancer Biother Radiopharm.
18 Schmitt A., Bernhardt P., Nilsson O., Ahlman H., Kolby L., Schmitt J., Forssel-Aronsson E. (2003). Biodistribution and dosimetry of 177Lu-labeled [DOTA0,Tyr3]octreotate in male nude mice with human small cell lung cancer. Cancer Biother Radiopharm.
19 Mena E., Camacho V., Estorch M., Fuertes J., Flotats A., Carrio I. (2004). 99mTc-depreotide scintigraphy of bone lesions in patients with lung cancer. Eur J Nucl Med Mol Imaging.
20 Martins T., Lino J.S., Ramos S., Oliveira L. (2004). 99mTc-depreotide scintigraphy in the evaluation of indeterminate pulmonary lesions: clinical experience. Cancer Biother Radiopharm.
21 Boundas D., Karatzas N., Moralidis E., Arsos G., Drevelengas A., Pistevou-Gompaki K., Karakatsanis C. (2007). Comparative evaluation of 99mTc-depreotide and 201Tl chloride single photon emission tomography in the characterization of pulmonary lesions. Nucl Med Commun.
22 Cholewinski W., Kowalczyk J.R., Stefaniak B., Stefaniak J., Poniatowicz-Frasunek E., Tarkowska A. (2004). Diagnosis and staging of children's lymphoma using the technetium-labelled somatostatin analogue, 99mTc-depreotide. Eur J Nucl Med Mol Imaging.
23 Papathanasiou N.D., Rondogianni P.E., Pianou N.K., Karampina P.A., Vlontzou E.A., Datseris I.E. (2008). 99mTc-depreotide in the evaluation of bone infection and inflammation. Nucl Med Commun.
24 Van Den Bossche B., D'Haeninck E., De Winter F., Van Belle S., Dierckx R.A., Van De Wiele C. (2004). 99mTc depreotide scan compared with 99mTc-MDP bone scintigraphy for the detection of bone metastases and prediction of response to hormonal treatment in patients with breast cancer. Nucl Med Commun.
25 Ferran N., Ricart Y., Lopez M., Martinez-Ballarin I., Roca M., Gamez C., Carrerea D., Guirao S., Leon A.F., Martin-Comin J. (2006). Characterization of radiologically indeterminate lung lesions: 99mTc-depreotide SPECT versus 18F-FDG PET. Nucl Med Commun.